# ^131^I-Tositumomab

Chemical name: | ^131^I-Tositumomab
Abbreviated name: | ^131^I-B1 MAb
Synonym: | Bexxar®, ^131^I-anti-CD20 antibody, ^131^I-anti-B1 antibody
Agent Category: | Antibody
Target: | CD20 antigen on B-cell non-Hodgkin’s lymphoma
Target Category: | Antibody-antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), gamma imaging
Source of signal/contrast: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=115968), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=29773) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=931) for more information about CD20.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22iodine-131%20anti-B1%20antibody%22%5BSubstance%20Name%5D%20OR%20Bexxar%5BText%20Word%5D%29%20OR%20tositumomab%5BAll%20Fields%5D)]

^131^I-Tositumomab (^131^I-B1 MAb) is a conjugation of ^131^I with a murine anti-CD20 monoclonal antibody (MAb) that can be used for both imaging and therapy of lymphoid malignancies (1-8). It was approved in the United States in 2003 for the therapeutic treatment of patients with relapsed, rituximab-refractory, CD20+, follicular non-Hodgkin’s lymphoma (NHL), with or without transformation.

The CD20 antigen (B1) is a 35-kDa, cell-surface nonglycosylated, hydrophobic phosphoprotein expressed on normal and malignant B cells, and it does not shed, modulate, or internalize (3, 7, 9). It is a transmembrane protein that acts as a calcium channel and plays an important role in cell cycle progression and differentiation of B cells. B1 is present on approximately 9% of the peripheral blood mononuclear cell fraction and >90% of B cells from blood and lymphoid organs. Lymphoma cells from >90% of patients with B cell NHL expressed this antigen. When antibodies bind to this antigen, they induce apoptosis, antibody-dependent cellular cytotoxicity, and complement-dependent cytotoxicity of lymphoma cells. Despite the presence of CD20 on normal B cells, it is a good tumor target for molecular targeting with antibodies for the management of NHL.

Radiolabeled MAbs have been developed for both diagnosis and therapy of tumors (3, 8, 10). Tositumomab (B1 MAb) was initially developed by the Dana-Farber Cancer Institute (8, 11). It is an intact murine IgG_2a_ lambda MAb directed against the CD20 antigen and is composed of two murine gamma 2a heavy chains of 451 amino acids each and two lambda light chains of 220 amino acids each (5, 12). ^131^I-B1 MAb has an approximate molecular weight of 150 kDa and is covalently linked to ^131^I. ^131^I emits both gamma and beta radiation, and it can be used for imaging at low doses and therapy at high doses (2). It is also relatively inexpensive and easy to conjugate to proteins. Although ^131^I-B1 MAb is only approved by the U.S. Food and Drug Administration for therapy, a dosimetric low dose of 185 MBq (5 mCi) has been used in the therapy protocol for whole-body imaging/counting on at least three occasions to determine unacceptable abnormal distribution and to establish the individualized therapeutic dose for a specific patient based on his/her tissue distribution and body clearance of ^131^I-B1 MAb.

The B1 MAb in the commercial preparation is produced in an antibiotic-free culture of mammalian cells and is supplied at a nominal concentration of 14 mg/ml of antibody (12). ^131^I-B1 MAb is supplied as a sterile, preservative-free liquid at nominal protein and activity concentrations of 0.1 mg/ml and 22.57 MBq (0.6 mCi)/ml (at the date of calibration), respectively. The formulation contains 4.4%-6.6% (w/v) providone, 1-2 mg/ml of maltose, 8.5-9.5 mg/ml of sodium chloride, and 0.9-1.3 mg/ml of ascorbic acid at pH 7.0.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Bexxar%20or%20Tositumomab%29%20AND%20synthesis)]

B1 MAb was synthesized based on the hybridoma technique developed by Kohler and Milstein (11, 13-16). The antibody was isolated from serum-free hybridoma supernatants and purified by ion-exchange chromatography to produce a preparation with >98% pure monomeric IgG. It was labeled with ^131^I using direct iodination methods (10, 16, 17). Several studies used the Iod-o-Gen method. The radiochemical yield was > 90% of radioactivity bound to the antibody, as measured by thin-layer chromatography The mean specific activities were reported to be 30.71-325.6 MBq (0.83-8.8 mCi)/mg. Other methods such as the chloramine-T method had also been used (18, 19). In 2003, Beeson and colleagues (11) demonstrated a new method that involved attaching the radioactive iodide to this antibody through a linker (cephalosporin) that could be cleaved in vivo by an administered enzyme (β-lactamase) for rapid clearance as a means to reduce patient radiation exposure.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

Stashenko and colleagues (20) in 1980 first reported the generation of a specific B1 MAb using the hybridoma technique. This MAb showed a 94.5% of absorption by human B cells from healthy volunteer donors. In 1991, ^125^I-B1 MAb supplied by the commercial source reported a mean binding affinity (K_d_) of 1.37 ± 0.22 nM (n=3) to a human CD20-expressing B-cell line (BALL-1) (1). In comparison, another anti-CD20 MAb (^125^I-rituximab) had a K_d_ of 4.36 ± 0.34 nM (n=3).

## Animal Studies

### Rodents

[PubMed]

Localization and imaging of radiolabeled B1 MAb were studied in nude mice bearing malignant CD20+ B-lymphoblastoid Namalwa tumors (21). Live cell radioimmunoassay indicated an 11.9% binding of ^125^I-B1 MAb to this human cell line. The mouse biodistribution of 18.5 kBq (0.5 µCi) of ^125^I-B1 MAb by i.p. injection showed tumor/blood ratios of 1.2 and 0.7 at 4 and 6 days after injection (n = 6-8), respectively. On the 6th day after injection, more than 5-fold greater activity was reported in tumor as compared with other soft tissue organs (liver, kidney, spleen, muscle). Imaging of 1.11 MBq (30 µCi) of ^131^I-B1 MAb in nude mice at 2 and 4 days after i.p. injection showed tumor/nontumor (T/NT) ratios of 0.33 and 0.39, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Bexxar%20or%20tositumomab%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

Radiolabeled B1 MAb was studied in rhesus monkeys at the New England Primate Research Center in 1987 (22). Approximately 18.5 MBq (0.5 mCi) of ^131^I-B1 MAb (0.3 ^131^I atom/MAb molecule) were administered i.v. to each monkey (n=2). One monkey received 2.0 mg of ^131^I-B1 MAb protein (high dose) and the other one received only 0.14 mg (low dose). Imaging of both animals 24 h after the infusions showed radioactivity primarily in the blood pool, heart and liver. The spleens (lymphocyte-rich) contained a high concentration of radioactivity, and the ratio of spleen to heart activity increased by 111% over a period of 5 days in the high-dose monkey and increased only 53% in the low-dose monkey. The serum clearance of total radioactivity was slightly more rapid in the high-dose animal (t½ = 24.1 h) than in the low-dose animal (t½ = 28.8 h). The cumulative urine excretions over 7 days were 33.6% and 28.7% for the low-dose monkey and high-dose monkey, respectively.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Bexxar%20or%20tositumomab%29%20AND%20human)]

A human pharmacokinetics study indicated that the half-life of ^131^I-B1 MAb was affected by the extent of disease of the patient. In 53 patients with different degrees of disease involvement, the mean body clearance (t_½_) was 68.9 h. Patients with splenomegaly had a t_½_ of 50 h and patients with greater disease burden had t_½_ of 68.0 hours. No change was found in patients with bone marrow involvement (1). In another study of 43 patients with B-cell lymphoma in relapse, the mean serum retention half-times of 185-370 MBq (5-10 mCi) of ^131^I-B1 MAb were 35.5 ± 16.8, 48.2 ± 17, and 48.1 ± 23.3 h after doses of 0.5 ± 2.5 and 10 mg/kg, respectively (23). Tumor uptake averaged 0.009 ± 0.003% injected dose/g of tumor in patients with favorable biodistribution (greater radiation doses to the tumors than other organs) and 0.002 ± 0.002% in patients with unfavorable biodistribution.

In a Phase I trial, increasing the predoses of unlabeled B1 MAb from 0 to 475 mg was associated with prolongation of the body clearance t_½_ of ^131^I-anti-B1-MAb from 63 to 85 h. The predosing with 475 mg of unlabeled B1 MAb appeared to provide superior tumor targeting (24). In another study with 685 mg of B1 MAb predosing and 185 MBq (5 mCi) in 15-20 mg of ^131^I-B1 MAb, definite tumor imaging was observed in all NHL CD20+ patients (n=34) with tumor sites larger than >2 cm. On average, the tumors received approximately 17 times the radiation dose delivered to the whole body (25).

Koral and colleagues (26) in 1994 demonstrated the use of computed tomography-single photon emission computed tomography (CT-SPECT) image fusion plus conjugate views to provide quantitative SPECT imaging of ^131^I-B1 MAb and to allow the quantification of tumor radioactivity in vivo. This hybrid SPECT-conjugate-view method was further refined, and a review of the results of 33 NHL patients who received 450 mg of B1 MAb predose and 185 MBq(5 mCi) of ^131^I-B1 MAb indicated that it could be used to provide radiation absorbed dose estimates of ^131^I-B1 MAb for the tumors in individual patient (27, 28).

On the basis of the sequential whole body imaging and the MIRDOSE 3 program, the median absorbed doses (mGy/MBq) of ^131^I-B1 MAb to the major organs were 2.71 (thyroid), 1.96 (kidneys), 1.3 (intestine walls), 1.25 (heart wall), 1.14 (spleen), and 0.65 (red marrow) (12). The critical organ appeared to be the bone marrow, because the dose-limiting toxicity was hematologic. The most common adverse reactions recorded during the clinical trials included neutropenia, thrombocytopenia, and anemia.

Various other studies have been published on the dosimetry and efficacy of the therapeutic application of treating NHL using high doses of ^131^I-B1 MAb [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Bexxar%20or%20tositumomab%29%20AND%20human%20and%20therapy%29)].

## Supplemental Information

### NIH Support

NIH DE-04881, AI 12069, CA 19589, CA 06516, RR 05526.

### References

1 (2003). Iodine-131 Tositumomab: (131)I-anti-B1 antibody, (131)I-tositumomab, anti-CD20 murine monoclonal antibody-I-131, B1, Bexxar, (131)I-anti-B1 antibody, iodine-131 tositumomab, iodine-131 anti-B1 antibody, tositumomab. BioDrugs.
2 Dillman R.O. (2002). Radiolabeled anti-CD20 monoclonal antibodies for the treatment of B-cell lymphoma. J Clin Oncol.
3 Hainsworth J.D. (2000). Monoclonal antibody therapy in lymphoid malignancies. Oncologist.
4 Hudson P.J. (2000). Design, production and evaluation of novel diagnostic and therapeutic reagents. 6-9 December 1999, La Jolla, CA, USA. IDrugs.
5 Lewington V. Development of 131I-tositumomab Semin Oncol 2005 32Suppl 11 S50 6 15786026
6 Milenic D.E., Brechbiel M.W. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
7 Tobinai K. (2003). Rituximab and other emerging antibodies as molecular target-based therapy of lymphoma. Int J Clin Oncol.
8 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
9 Zelenetz A.D. A clinical and scientific overview of tositumomab and iodine I 131 tositumomab Semin Oncol 2003 30Suppl 42 22 30 12728404
10 Kowalsky R.J., Falen S.W. (2004). Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. , Washington, D.C.: APhA. 733-752.
11 Stashenko P., Nadler L.M., Hardy R., Schlossman S.F. (1980). Characterization of a human B lymphocyte-specific antigen. The Journal of Immunology.
12. Bexxar (Tositumomab and Iodine I 131 Tositumomab) Package Insert RL-2245. 2005, GlaxoSmithKline. p. 1-33.
13 Kohler G., Milstein C. (1975). Continuous cultures of fused cells secreting antibody of predefined specificity. Nature.
14 Campbell P., Marcus R. (2003). Monoclonal antibody therapy for lymphoma. Blood Rev.
15 Cheson B. (2002). Bexxar (Corixa/GlaxoSmithKline). Curr Opin Investig Drugs.
16 Kaminski M.S., Zasadny K.R., Francis I.R., Milik A.W., Ross C.W., Moon S.D., Crawford S.M., Burgess J.M., Petry N.A., Butchko G.M., et al. (1993). Radioimmunotherapy of B-cell lymphoma with [131I]anti-B1 (anti-CD20) antibody. N Engl J Med.
17 Fraker P.J., Speck J.C. (1978). Protein and cell membrane iodinations with a sparingly soluble chloroamide, 1,3,4,6-tetrachloro-3a,6a-diphrenylglycoluril. Biochem Biophys Res Commun.
18 Eary J.F., Press O.W., Badger C.C., Durack L.D., Richter K.Y., Addison S.J., Krohn K.A., Fisher D.R., Porter B.A., Williams D.L., et al. (1990). Imaging and treatment of B-cell lymphoma. J Nucl Med.
19 Beeson C., Butrynski J.E., Hart M.J., Nourigat C., Matthews D.C., Press O.W., Senter P.D., Bernstein I.D. (2003). Conditionally cleavable radioimmunoconjugates: a novel approach for the release of radioisotopes from radioimmunoconjugates. Bioconjug Chem.
20 Cardarelli P.M., Quinn M., Buckman D., Fang Y., Colcher D., King D.J., Bebbington C., Yarranton G. (2002). Binding to CD20 by anti-B1 antibody or F(ab')(2) is sufficient for induction of apoptosis in B-cell lines. Cancer Immunol Immunother.
21 Buchsbaum D.J., Sinkule J.A., Stites M.S., Fodor P.A., Hanna D.E., Ford S.M., Warber-Matich S.L., Juni J.E., Foon K.A. (1988). Localization and imaging with radioiodine-labeled monoclonal antibodies in a xenogeneic tumor model for human B-cell lymphoma. Cancer Res.
22 Letvin N.L., Zalutsky M.R., Lambert J.M., Chalifoux L.V., Nadler L.M., Schlossman S.F., Atkins H.L. (1987). Use of radiolabeled monoclonal anti-B1 antibody for B lymphocyte imaging in rhesus monkeys. Int J Rad Appl Instrum B.
23 Press O.W., Eary J.F., Appelbaum F.R., Martin P.J., Badger C.C., Nelp W.B., Glenn S., Butchko G., Fisher D., Porter B., et al. (1993). Radiolabeled-antibody therapy of B-cell lymphoma with autologous bone marrow support. N Engl J Med.
24 Cheson B.D. (2003). Radioimmunotherapy of non-Hodgkin lymphomas. Blood.
25 Kaminski M.S., Zasadny K.R., Francis I.R., Fenner M.C., Ross C.W., Milik A.W., Estes J., Tuck M., Regan D., Fisher S., Glenn S.D., Wahl R.L. (1996). Iodine-131-anti-B1 radioimmunotherapy for B-cell lymphoma. J Clin Oncol.
26 Koral K.F., Zasadny K.R., Kessler M.L., Luo J.Q., Buchbinder S.F., Kaminski M.S., Francis I., Wahl R.L. (1994). CT-SPECT fusion plus conjugate views for determining dosimetry in iodine-131-monoclonal antibody therapy of lymphoma patients. J Nucl Med.
27 Koral K.F., Dewaraja Y., Li J., Barrett C.L., Regan D.D., Zasadny K.R., Rommelfanger S.G., Francis I.R., Kaminski M.S., Wahl R.L. (2000). Initial results for Hybrid SPECT--conjugate-view tumor dosimetry in 131I-anti-B1 antibody therapy of previously untreated patients with lymphoma. J Nucl Med.
28 Koral K.F., Dewaraja Y., Li J., Lin Q., Regan D.D., Zasadny K.R., Rommelfanger S.G., Francis I.R., Kaminski M.S., Wahl R.L. (2003). Update on hybrid conjugate-view SPECT tumor dosimetry and response in 131I-tositumomab therapy of previously untreated lymphoma patients. J Nucl Med.